# ^99m^Tc-Labeled 6-hydrazinopyridine-3-carboxylic acid conjugated to hydroxy-bisphosphonate

Chemical name: | ^99m^Tc-Labeled 6-hydrazinopyridine-3-carboxylic acid conjugated to hydroxy-bisphosphonate
Abbreviated name: | [^99m^Tc]HYNIC-HBP
Synonym:
Agent Category: | Compound
Target: | Farnesyl disphosphate synthase
Target Category: | Enzyme
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure of [^99m^Tc]HYNIC-HBP for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=bisphosphonates&cmd=DetailsSearch)]

Bisphosphonates (BPs) or nitrogen-containing bisphosphonates (NBPs) are often used for the management of pain palliation and disorders related to skeletal tissue, including those arising from cancer metastases, because these compounds exhibit a very high affinity for hydroxyapatite (HA), a component of the bone matrix (1). The NBPs tend to accumulate in osteoclasts at areas of increased bone metabolism by inhibiting the farnesyl diphosphate synthase, an important enzyme of the mevalonate pathway in the cell (2). Several BPs and NBPs are available commercially for clinical use to treat different bone disorders, and there are ongoing clinical trials (http://clinicaltrials.gov/ct2/results?term=bisphosphonates) approved by the United States Food and Drug Administration to evaluate these compounds for the treatment of various bone ailments. In addition, BPs are often labeled with ^99m^Tc or ^186/188^Re and used for the imaging and treatment of bone metastases. However, these compounds have limitations primarily because they either exist as a mixture of anionic compounds with varying properties (e.g., [^99m^Tc]-labeled methylene-diphosphonate (MDP) or [^99m^Tc]-labeled hydroxymethylene-diphosphonate (HMDP)) or are rapidly degraded (e.g., [^186/188^Re]MDP) under in vivo conditions, resulting in a reduced uptake at targeted bone areas and an increased accumulation in non-target soft tissue (3). The ^99m^Tc- or ^186/188^Re-labeled BPs were suggested to have these limitations because the compounds possess dual activities: one phosphonate group of the BP molecule acts as a radionuclide chelator, and the other phosphonate group binds to the target(s). Therefore, due to close proximity of the two groups, one activity may be interfering with the other (3).

To circumvent problems associated with the radiolabeled BPs, investigators developed NBPs with two independent activities such that the nitrogen-containing part would only chelate the radiotracer and the BP part would target the bone (4). Ogawa et al. synthesized and labeled two NBPs, 6-hydrazinopyridine-3-carboxylic acid-hydroxy-bisphosphonate (HYNIC-HBP) and mercaptoacetylglycylglycylglycine-hydroxy-bisphosphonate (MAG3-HBP), with ^99m^Tc to obtain [^99m^Tc]HYNIC-HBP and [^99m^Tc]MAG3-HBP (4). The two imaging agents were valuated for binding to hydroxyapatite (HA) under in vitro conditions and for bone scintigraphy in normal rats (4). This chapter presents the studies performed and the results obtained with [^99m^Tc]HYNIC-HBP. The in vitro and in vivo studies and the results obtained with [^99m^Tc]MAG3-HBP are presented in a separate chapter in MICAD (www.micad.nih.gov) (5).

### Other sources of information

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001037277.1) of human farnesyl diphosphate synthase

Gene information (http://www.ncbi.nlm.nih.gov/gene/2224) regarding human farnesyl diphosphate synthase (GeneID: 2224)

Farnesyl diphosphate synthase in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/134629)

Structure of farnesyl diphosphate synthase (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=59201) complexed with a bisphosphonate

Farnesyl diphosphate synthase in Kyoto Encyclopedia of Genes and Genomes (KEGG) Pathways (http://www.genome.jp/dbget-bin/www_bget?pathway+hsa00900)

Related chapters (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Farnesyl+diphosphate+synthase++AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=dipicolylamine-alendronate%20synthesis&cmd=DetailsSearch)]

The synthesis, characterization, and ^99m^Tc labeling of HYNIC-HBP were described by Ogawa et al. (4). The labeled product had a radiochemical yield of 39% and a purity of >95% as determined with reverse-phase high-performance liquid chromatography. The specific activity of the radiolabeled compound was not reported.

The production, radiochemical purity, yield, stability, and specific activity of [^99m^Tc]HMDP, used for comparison in some of the studies, were not reported (4).

As determined in serum isolated from rats injected with the respective radiotracers, 97.7 ± 0.2% of [^99m^Tc]HYNIC-HBP was reported to bind to serum proteins compared with 88.7 ± 2.7% for [^99m^Tc]MAG3-HBP. The serum binding of [^99m^Tc]HMDP was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=technetium%2099m%206-hydrazinopyridine-3-carboxylic%20acid-hydroxybisphosphonate%20AND%20in%20vitro&cmd=DetailsSearch)]

An in vitro assay was used to compare the HA binding of ^99m^Tc-labeled HYNIC-HBP, MAG3-HBP, and HMDP, respectively (4). Among these labeled compounds, both [^99m^Tc]HYNIC-HBP and [^99m^Tc]MAG3-HBP bound to a similar level with HA, and the binding was significantly higher (P < 0.05) than that exhibited by [^99m^Tc]HMDP (for details see Figure 2 in Ogawa et al. (4)).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=dipicolylamine-alendronate%20rodentia&cmd=DetailsSearch)]

Ogawa et al. investigated the biodistribution of [^99m^Tc]HYNIC-HBP, [^99m^Tc]MAG3-HBP, and [^99m^Tc]HMDP in normal rats (4). The rats were given an intravenous injection of the respective radiotracers (n = 4–6 animals/time point for each radiotracer), and the animals were euthanized at predetermined time points up to 60 min after treatment. Organs of interest were removed from the euthanized animals and counted for accumulated radioactivity, and the data were presented as percent injected dose per gram tissue (%ID/g). The amount of radioactivity in blood from [^99m^Tc]HYNIC-HBP, [^99m^Tc]MAG3-HBP, and [^99m^Tc]HMDP decreased from 0.56 ± 0.05% ID/g, 0.98 ± 0.09% ID/g, and 0.61 ± 0.03% ID/g at 5 min to 0.03 ± 0.01% ID/g, 0.07 ± 0.01% ID/g, and 0.04 ± 0.01% ID/g at 60 min after injection, respectively. A similar pattern of decreased radioactivity in the kidneys was reported with the three tracers, indicating that the label was eliminated from the animals through the urinary route. The femur (the only bone reported to have been removed from the rats) showed [^99m^Tc]HYNIC-HBP, [^99m^Tc]MAG3-HBP, and [^99m^Tc]HMDP radioactivity uptake values of 1.90 ± 0.21% ID/g, 1.80 ± 0.24% ID/g, and 1.52 ± 0.14% ID/g at 5 min, respectively, which increased to 3.96 ± 0.36% ID/g, 4.23 ± 0.25% ID/g, and 3.13 ± 0.51% ID/g at 60 min after injection, respectively. The femur/blood ratios at 60 min were 123 ± 18.30, 59.7 ± 10.41, and 93.40 ± 19.81 for [^99m^Tc]HYNIC-HBP, [^99m^Tc]MAG3-HBP, and [^99m^Tc]HMDP, respectively, which indicated that [^99m^Tc]HYNIC-HBP was superior to [^99m^Tc]MAG3-HBP and [^99m^Tc]HMDP for binding to the bone.

On the basis of the above observations, the investigators concluded that [^99m^Tc]HYNIC-HBP is a good bone targeting agent and has potential as a bone scintigraphy agent (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-HYNIC-HBP%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-HYNIC-HBP%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-HYNIC-HBP%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Drake M.T., Clarke B.L., Khosla S. (2008). Bisphosphonates: mechanism of action and role in clinical practice. Mayo Clin Proc.
2 Kimmel D.B. (2007). Mechanism of action, pharmacokinetic and pharmacodynamic profile, and clinical applications of nitrogen-containing bisphosphonates. J Dent Res.
3 Torres Martin de Rosales R., Finucane C., Mather S.J., Blower P.J. (2009). Bifunctional bisphosphonate complexes for the diagnosis and therapy of bone metastases. Chem Commun (Camb).
4 Ogawa K., Mukai T., Inoue Y., Ono M., Saji H. (2006). Development of a novel 99mTc-chelate-conjugated bisphosphonate with high affinity for bone as a bone scintigraphic agent. J Nucl Med.
5 Chopra, A., [99mTc]Labeled mercaptoacetlyglycylglycylglycine conjugated to hydroxy-bisphosphonate. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.